# Chlorotoxin:Cy5.5

Chemical name: | Chlorotoxin:Cy5.5
Abbreviated name: | CTX:Cy5.5
Synonym: | Tumor paint
Agent Category: | Peptide
Target: | Matrix metalloproteinase 2 (MMP2)
Target Category: | Enzyme-substrate binding
Method of detection: | Near infrared (NIR)
Source of signal: | Cy5.5
Activation: | Not required
Studies: | - In vitro; - Rodents | Structure of Chlorotoxin:Cy5.5.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Chlorotoxin%3Acy5.5)]

Chlorotoxin (CTX) is a neurotoxin comprising 36 amino acids and is isolated from the venom of Leiurus quinquestriatus, a scorpion of the Buthidae family. A characteristic feature of the peptide is that it contains four disulfide bonds that give it a tight tertiary structure and a single tyrosine residue that can be iodinated. Originally, CTX was described as a calcium channel blocker (1) that was later shown to bind specifically to isoform 2 of a matrix metalloproteinase (MMP2) associated with the channels (2). The MMP2 was shown to be upregulated in many cancers, especially glioblastomas, and there appears to be a correlation between the level of MMP2 expression and poor outcome of the disease (1-6). For most neoplastic conditions, a surgical resection of affected tissue is the most common treatment, and the precision of this technique can influence patient prognosis. The identification and removal of tumors is largely based on a surgical judgment and can be imprecise because it involves avoiding the removal of normal or apparently healthy tissue. Incomplete removal of cancer cells is a problem often encountered with brain tumors, and >80% of malignant cancers recur at the site of tumor removal (7). Clear distinction of tumor tissue from normal tissue could alleviate the problem of incomplete removal of cancer tissue by surgical resection and help improve patient prognosis. The development of agents that bind to tumor-specific molecules and their use to illuminate tumor cells during surgery would greatly facilitate the achievement of this goal.

Biocompatible fluorescent contrast agents conjugated to peptides, proteins, or antibodies, including those visible with near infrared (NIR) light, have been developed and evaluated for the optical imaging of tumors (8, 9). These agents can be used for non-invasive or intraoperative imaging because water or hemoglobin do not absorb in the NIR spectrum and allow the photons to penetrate the tissue. The use of a cyanine (Cy) dye conjugated to a variety of molecules has been explored to image various cancers (10). From these studies it was concluded that small peptides offer a greater advantage over large molecules, e.g., antibodies, because they are easy to synthesize and modify, are likely to be less immunogenic, can be rapidly cleared from circulation, and rapidly accumulate in the target area to give a high signal/background ratio.

Brain tumor imaging has been performed with NIR probes that targeted tumor microglia or required proteolytic activation (11, 12). However, the former approach does not always correlate with detection of the brain tumor margins because patients are often treated with dexamethasone, an inhibitor of microglia activation, to reduce post-operative edema. Previously, a multifunctional probe fabricated with iron oxide nanoparticles coated with covalently bound bifunctional polyethylene glycol, CTX, and Cy5.5 was developed and successfully used invitro to image glioma cells (13). CTX and Cy5.5 are available commercially in the United States. Fluorescence microscopy and magnetic resonance imaging showed that conjugated nanoparticles were taken up preferentially by the glioma cells. From observations made during the study, the potential use of the conjugate for real-time imaging of glioma brain tumors was suggested. Subsequently, Veiseh et al. developed and evaluated a CTX:Cy5.5 dye bioconjugate that requires no protease activation to image neoplastic tumors in a mouse model (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CTX%3ACy5.5+synthesis)]

The synthesis of CTX:Cy5.5 was described by Veiseh et al. (14). Both CTX and the Cy5.5 dye (as an ester) were purchased from commercial sources. The Cy5.5 dye was dissolved in anhydrous dimethyl formamide and mixed with a CTX solution in bicarbonate buffer (pH 8.5) at a ratio of 3:1. The conjugation was allowed to proceed for 1 h at room temperature in the dark. Excess dye was removed by dialysis against phosphate-buffered saline (PBS) for 18 h at 4°C. The samples were diluted in PBS to various appropriate dilutions and filter-sterilized for use in the different studies. Quality of the conjugated product was monitored by mass spectroscopy. The yields, purity, and Cy5.5/CTX ratio of the conjugated product were not provided in the publication.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=chlorotoxin%3ACy5.5+in+vitro)]

For in vitro evaluation of CTX:Cy5.5, 9L glioma cells and primary fibroblasts (as controls) were exposed to the same concentration of the bioconjugated agent under identical conditions and the binding was visualized by NIR fluorescence (NIRF) microscopy (14). All the 9L glioma cells exposed to the probe emitted a signal in the NIRF spectrum, and a minimal signal was detected with the fibroblasts. It was also observed that the MMP2 inhibitor 1,10-phenanthroline blocked the binding of CTX:Cy5.5 to the 9L glioma cells, which indicated that the CTX:Cy5.5 bioconjugate bound specifically to the metalloproteinase.

In another study to show that MMP2 is specifically involved in the binding of CTX:Cy5.5, MCF7 cells known to express low levels of MMP2 and bond CTX:Cy5.5 poorly compared to the other cell lines were transfected with a plasmid encoding the MMP2 (14). Cells expressing the MMP2 were sorted from the untransfected cells and an increased expression of the proteinase in these cells was confirmed by indirect immunofluorescence, Western blot analysis, and gelatinase assays. Although no signal/noise ratios were provided by the investigators, from image analysis it was clear the MMP2-transfected cells showed higher CTX:Cy5.5 binding compared to control cells transfected with the control plasmid (which contained no MMP2 insert). This again confirmed that CTX:Cy5.5 bound specifically to MMP2.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=chlorotoxin%3ACy5.5+rodentia)]

The in vivo activity of CTX:Cy5.5 was investigated non-invasively by injecting the bioconjugate into mice bearing 9L glioma xenografts (14). The NIRF signal was significantly higher in all xenografts compared to the non-neoplastic tissue at all time points through day 14. Also, mice bearing 9L glioma cell flank xenografts showed a significantly increased NIRF signal compared to that observed in the brain at all time points tested. To investigate the specificity of the CTX:Cy5.5 signal from the tumors, the probe was coadministered with CTX to mice bearing the xenografts. With the use of biophotonic imaging, CTX was observed to block the binding of CTX:Cy5.5 to the tumors. In another study, Cy5.5 alone was administered to the mice bearing xenografts and, for comparison, another group of the same mice received the bioconjugate alone. The NIRF signals obtained from the tumors of these two groups of mice were compared. With the use of imaging it was observed that mice injected with the probe had a significantly higher tumor signal/noise ratio (from ~15-fold higher at day 1 to four-fold higher at day 4 after the injection) compared to mice injected with Cy5.5 alone. A similar distinction was observed between tumors and normal tissue in a brain xenograft model. This distinction showed that CTX:Cy5.5 bound specifically to the neoplastic tissue and did not bind to the surrounding, normal, healthy tissue.

Imaging studies were also conducted to determine whether CTX:Cy5.5 illuminated cancer foci of MMP2-positive tumors that were not of neuroectodermal origin (14). Transgenic mice that expressed the SV40T gene in the prostate epithelium (15) were injected with CTX:Cy5.5. The probe was observed to illuminate the primary prostate cancer as well as metastatic tissue in the lungs. It was also reported that the microscopic foci of cancer cells in the lymphatic channels and the lymph nodes of the animals were easily detected under simulated surgical conditions. A similar study was performed with mice bearing Rh30 rhabdomyosarcoma xenografts. The investigators observed that CTX:Cy5.5 targeted the tumor specifically compared to the normal surrounding tissue in this model as well. Presence of cancer cells in the tumors or absence of cancer cells in the normal tissue, as distinguished by the use of CTX:Cy5.5, was also confirmed by pathological examination. These studies demonstrated that CTX:Cy5.5 could help clearly distinguish cancerous tissue from normal tissue under simulated operating conditions.

The tissue distribution of CTX:Cy5.5 was also studied (14). The unbound bioconjugate was fairly evenly distributed through the mouse body, except in the renal collecting system, up to 96 hours after administration. The renal collecting system had a high NIRF signal compared to the other organs because the bioconjugate is excreted in the urine.

From these studies, the long duration (up to 14 days) of probe activity allowed tumor imaging even after the peak circulating levels had dropped significantly. The clear distinction of tumors from normal tissues led the investigators to conclude that CTX:Cy5.5 could be a good probe for the detection of neoplastic cells during surgery to remove tumors from human patients.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=chlorotoxin%3ACy5.5+Non-Primate+Mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=chlorotoxin%3ACy5.5+Non-Human+Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=chlorotoxin%3ACy5.5+Human+studies)]

No publications are currently available.

## References

1 Soroceanu L., Gillespie Y., Khazaeli M.B., Sontheimer H. (1998). Use of chlorotoxin for targeting of primary brain tumors. Cancer Res.
2 Deshane J., Garner C.C., Sontheimer H. (2003). Chlorotoxin inhibits glioma cell invasion via matrix metalloproteinase-2. J Biol Chem.
3 Sakakibara M., Koizumi S., Saikawa Y., Wada H., Ichihara T., Sato H., Horita S., Mugishima H., Kaneko Y., Koike K. (1999). Membrane-type matrix metalloproteinase-1 expression and activation of gelatinase A as prognostic markers in advanced pediatric neuroblastoma. Cancer.
4 Kanayama H., Yokota K., Kurokawa Y., Murakami Y., Nishitani M., Kagawa S. (1998). Prognostic values of matrix metalloproteinase-2 and tissue inhibitor of metalloproteinase-2 expression in bladder cancer. Cancer.
5 Davidson B., Goldberg I., Kopolovic J., Lerner-Geva L., Gotlieb W.H., Ben-Baruch G., Reich R. (1999). MMP-2 and TIMP-2 expression correlates with poor prognosis in cervical carcinoma--a clinicopathologic study using immunohistochemistry and mRNA in situ hybridization. Gynecol Oncol.
6 Chambers A.F., Matrisian L.M. (1997). Changing views of the role of matrix metalloproteinases in metastasis. J Natl Cancer Inst.
7 Barker F.G., Chang S.M., Gutin P.H., Malec M.K., McDermott M.W., Prados M.D., Wilson C.B. (1998). Survival and functional status after resection of recurrent glioblastoma multiforme. Neurosurgery.
8 Bremer C., Ntziachristos V., Weissleder R. (2003). Optical-based molecular imaging: contrast agents and potential medical applications. Eur Radiol.
9 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
10 Tung C. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
11 Kircher M.F., Mahmood U., King R.S., Weissleder R., Josephson L. (2003). A multimodal nanoparticle for preoperative magnetic resonance imaging and intraoperative optical brain tumor delineation. Cancer Res.
12 Ntziachristos V., Tung C.H., Bremer C., Weissleder R. (2002). Fluorescence molecular tomography resolves protease activity in vivo. Nat Med.
13 Veiseh O., Sun C., Gunn J., Kohler N., Gabikian P., Lee D., Bhattarai N., Ellenbogen R., Sze R., Hallahan A., Olson J., Zhang M. (2005). Optical and MRI multifunctional nanoprobe for targeting gliomas. Nano Lett.
14 Veiseh M., Gabikian P., Bahrami S.B., Veiseh O., Zhang M., Hackman R.C., Ravanpay A.C., Stroud M.R., Kusuma Y., Hansen S.J., Kwok D., Munoz N.M., Sze R.W., Grady W.M., Greenberg N.M., Ellenbogen R.G., Olson J.M. (2007). Tumor paint: a chlorotoxin:cy5.5 bioconjugate for intraoperative visualization of cancer foci. Cancer Res.
15 Huss W.J., Maddison L.A., Greenberg N.M. (2001). Autochthonous mouse models for prostate cancer: past, present and future. Semin Cancer Biol.